# Quenched indocyanine green-anti-prostate-specific membrane antigen antibody J591

Chemical name: | Quenched indocyanine green-anti-prostate-specific membrane antigen antibody J591
Abbreviated name: | ICG-J591, J591-ICG
Synonym:
Agent category: | Antibody
Target: | Prostate-specific membrane antigen (PSMA), or N-acetyl α-linked acidic dipeptidase (NAALADase)
Target category: | Antigen
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | Indocyanine green (ICG)
Activation: | Yes
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4758398), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4758397) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2346) for more information about PSMA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a noninvasive alternative to radionuclide imaging in small animals or with probes in close proximity to the target in humans (4). Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment. It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumor cells and endoscopic imaging of the pancreas and colon.

Prostate-specific membrane antigen (PSMA) is a cell-surface glycoprotein with a molecular weight of ~100 kDa. It is a unique, type II, transmembrane-bound glycoprotein that is overexpressed on prostate tumor cells and in the neovasculature of most solid prostate tumors but not in the vasculature of normal tissues (5, 6). This unique expression of PSMA makes it an important biomarker as well as a large extracellular target of imaging agents (7, 8). PSMA has also been detected in other tissues such as the kidneys, the proximal small intestine, and the salivary glands (6). PSMA was found to have N-acetyl α-linked acidic dipeptidase (NAALADase) or glutamate carboxypeptidase II activity (9). PSMA may play an important role in the progression of prostate cancer and glutamatergic neurotransmission, as well as in the absorption of folate (10). In the central nervous system, PSMA metabolizes N-acetyl-aspartyl-glutamate, and in the proximal small intestine it removes γ-linked glutamates from poly-γ-glutamate folate and folate hydrolase (6). PSMA can be used as a marker for the detection of metastatic cancers with imaging agents. Although the commercially available monoclonal antibody ^111^In-labeled Capromomab pendetide (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Capromab111In) (^111^In-CYT-356) is in clinical use for the detection of prostate cancer, the results obtained with this antibody are not entirely reliable (11). In addition, this antibody has limited access to tumors and may produce low signal/noise ratios because the target is the intracellular domain of PSMA (12, 13). J591, a humanized monoclonal antibody against the extracellular domain of PSMA (14), was conjugated to QD655 (QD655-J591) and was found to accumulate in a human prostate cancer cell line in vitro and in nude mice (15). However, QD655-J591 has suboptimal tissue penetration and autofluorescence from the skin. To improve this approach, Shi et al. (16) used an anti-PSMA antibody J591conjugate with QDs (QD800-J591), which emit light in the NIR 800-nm range.

ICG loses its fluorescence upon conjugation to proteins (17). Ogawa et al. (18) utilized this unique property of ICG to create activatable optical probes with ICG-antibody conjugates. ICG (and thus fluorescence) was released from the targeting antibodies after cell-binding and internalization. Nakajima et al. (19) prepared quenched ICG-anti-PSMA antibody J591 (ICG-J591) for in vivo NIR imaging of PSMA-positive tumors in mice.

### Related Resource Links:

- Chapters in MICAD (PSMA (http://www.ncbi.nlm.nih.gov/books?term=PSMA%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D), J591 (http://www.ncbi.nlm.nih.gov/books?term=J591%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (PSMA (http://www.ncbi.nlm.nih.gov/gene/2346))
- Articles in Online Mendelian Inheritance in Man (OMIM) (PSMA (http://www.ncbi.nlm.nih.gov/omim/600934))
- Clinical trials (J591 (http://www.clinicaltrials.gov/ct2/results?term=J591), ICG (http://www.clinicaltrials.gov/ct2/results?term=ICG))
- Drug information in FDA (J591 (http://google2.fda.gov/search?q=j591&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=8), ICG (http://google2.fda.gov/search?q=Indocyanine+Green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ICG-J591)]

J591 (6.2 nmol) was incubated with ICG-sulfo-OSu (50 nmol) in Na_2_HPO_4_ buffer (pH 8.5) for 30 min at room temperature (19). ICG-J591 was purified with column chromatography. ICG-Trastuzumab (ICG-Tra) was similarly prepared. J591 was also conjugated with IR700DX N-hydroxysuccinimide ester. The number of ICG per antibody molecule was ~1 and ~3 for IR700. The immunoreactivity of ICG-J591 was 69% compared with 76% for J591. Sodium dodecyl sulfate polyacrylamide gel electrophoresis (SDS-PAGE) demonstrated that 70% of ICG was covalently linked to the antibody. Fluorescence intensity was low for both ICG-J591 and ICG-Tra in their native states, whereas exposure to 1% SDS showed an 18-fold and 15-fold increase in fluorescence intensity, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ICG%20J591%20and%20in%20vitro)]

LNCaP human prostate cancer cells were reported to have a binding affinity (K_d_) of 1.8 nM with ^131^I-labeled J591 and a B_max_ of 600,000–800,000 sites/cell in a saturation binding assay (14). Using a PSMA-transfected PC3 cell line (PC3-PSMA^+^) and a control cell line (PC3-PSMA^–^), saturation binding studies showed that ^125^I-labeled ICG-J591 and ^125^I-labeled J951 exhibited a similar K_d_ value of 2.8 nM with ~2 × 10^6^ binding sites/PC3-PSMA^+^ cell. Fluorescence microscopy and flow cytometry showed that IR700-J591 binding strongly to PC3-PSMA^+^ cells and only weakly to PC3-PSMA^–^ cells (19). The binding of IR700-J591 to PC3-PSMA^+^ cells was blocked by 100-fold excess of J591, whereas little inhibition was observed in PC3-PSMA^–^ cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ICG-J591%20and%20rodentia)]

Tumor-imaging studies of ICG-J591 were performed in nude mice (the number of mice was not reported) bearing PC3-PSMA^+^ and PC3-PSMA^–^ tumors on opposite dorsum (19). Whole-body fluorescence images were obtained at 0.25, 1, 2, 3, 4, 6, and 10 d after intravenous injection of ICG-J591 (0.04, 0.08, 0.16, and 0.32 nmol/mouse). Maximum NIR fluorescence signals (dose-dependent) in PC3-PSMA^+^ tumors were obtained at 1 day after injection for the four doses. There were only weak signals in PC3-PSMA^–^ tumors. The signal intensity ratio of PC3-PSMA^+^ to PC3-PSMA^–^ was ~14 at 4 d after injection of 0.04 nmol ICG-J591. PC3-PSMA^+^ tumors were clearly visualized even at 10 d after injection. No blocking studies (with unconjugated J591) were performed. Injection of 0.08 nmol ICG-Tra exhibited approximately two-fold lower fluorescence signals in 3T3HER2^+^ tumors as compared with the same dose of ICG-J591 in PC3-PSMA^+^ tumors. Both cell types exhibited a similar number of their respective receptors. The difference in tumor signals may be due to differences in the antibody delivery to tumors and/or the rates of internalization/activation in the tumor cells.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ICG-J591%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ICG-J591%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ICG%20J591%20and%20human)]

No publication is currently available.

## Human Studies

Intramural Research Program

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
5 Feneley M.R., Jan H., Granowska M., Mather S.J., Ellison D., Glass J., Coptcoat M., Kirby R.S., Ogden C., Oliver R.T., Badenoch D.F., Chinegwundoh F.I., Nargund V.H., Paris A.M., Britton K.E. (2000). Imaging with prostate-specific membrane antigen (PSMA) in prostate cancer. Prostate Cancer Prostatic Dis.
6 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
7 Nanus, D.M., M.I. Milowsky, L. Kostakoglu, P.M. Smith-Jones, S. Vallabahajosula, S.J. Goldsmith, and N.H. Bander, Clinical use of monoclonal antibody HuJ591 therapy: targeting prostate specific membrane antigen. J Urol, 2003170(6 Pt 2): p. S84-8; discussion S88-9.
8 Nargund V., Al Hashmi D., Kumar P., Gordon S., Otitie U., Ellison D., Carroll M., Baithun S., Britton K.E. (2005). Imaging with radiolabelled monoclonal antibody (MUJ591) to prostate-specific membrane antigen in staging of clinically localized prostatic carcinoma: comparison with clinical, surgical and histological staging. BJU Int.
9 Luthi-Carter R., Barczak A.K., Speno H., Coyle J.T. (1998). Molecular characterization of human brain N-acetylated alpha-linked acidic dipeptidase (NAALADase). J Pharmacol Exp Ther.
10 Yao V., Berkman C.E., Choi J.K., O'Keefe D.S., Bacich D.J. (2010). Expression of prostate-specific membrane antigen (PSMA), increases cell folate uptake and proliferation and suggests a novel role for PSMA in the uptake of the non-polyglutamated folate, folic acid. Prostate.
11 Ponsky L.E., Cherullo E.E., Starkey R., Nelson D., Neumann D., Zippe C.D. (2002). Evaluation of preoperative ProstaScint scans in the prediction of nodal disease. Prostate Cancer Prostatic Dis.
12 Sundaresan G., Yazaki P.J., Shively J.E., Finn R.D., Larson S.M., Raubitschek A.A., Williams L.E., Chatziioannou A.F., Gambhir S.S., Wu A.M. (2003). 124I-labeled engineered anti-CEA minibodies and diabodies allow high-contrast, antigen-specific small-animal PET imaging of xenografts in athymic mice. J Nucl Med.
13 Jain R.K. (1999). Transport of molecules, particles, and cells in solid tumors. Annu Rev Biomed Eng.
14 Smith-Jones P.M., Vallabahajosula S., Goldsmith S.J., Navarro V., Hunter C.J., Bastidas D., Bander N.H. (2000). In vitro characterization of radiolabeled monoclonal antibodies specific for the extracellular domain of prostate-specific membrane antigen. Cancer Res.
15 Gao X., Cui Y., Levenson R.M., Chung L.W., Nie S. (2004). In vivo cancer targeting and imaging with semiconductor quantum dots. Nat Biotechnol.
16 Shi C., Zhu Y., Xie Z., Qian W., Hsieh C.L., Nie S., Su Y., Zhau H.E., Chung L.W. (2009). Visualizing human prostate cancer cells in mouse skeleton using bioconjugated near-infrared fluorescent quantum dots. Urology.
17 Tadatsu Y., Muguruma N., Ito S., Tadatsu M., Kusaka Y., Okamoto K., Imoto Y., Taue H., Sano S., Nagao Y. (2006). Optimal labeling condition of antibodies available for immunofluorescence endoscopy. J Med Invest.
18 Ogawa M., Kosaka N., Choyke P.L., Kobayashi H. (2009). In vivo molecular imaging of cancer with a quenching near-infrared fluorescent probe using conjugates of monoclonal antibodies and indocyanine green. Cancer Res.
19 Nakajima T., Mitsunaga M., Bander N.H., Heston W.D., Choyke P.L., Kobayashi H. (2011). Targeted, activatable, in vivo fluorescence imaging of prostate-specific membrane antigen (PSMA) positive tumors using the quenched humanized J591 antibody-indocyanine green (ICG) conjugate. Bioconjug Chem.